# 5-[3-Hydroxy-2-hydroxymethyl-propionamido)-N,N´-dimethyl-N,N´-bis-(2,3-dihydroxypropyl)-2,4,6-triiodoisophthalamide

Chemical name: | 5-[3-Hydroxy-2-hydroxymethyl-propionamido]-N-N´-dimethyl-N-N´-bis-(2,3-dihydroxypropyl)-2,4,6-triiodoisophthalamide
Abbreviated name: | Iobitridol
Synonym: | Xenetix^®^
Agent Category: | Compound
Target: | Non-targeted agent, blood pool, extracellular space
Target Category: | Non-targeted filling of blood vessels and organs
Method of detection: | X-ray, CT
Source of signal/contrast: | Iodine (I)
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Iobitridol%20OR%20Xenetix)]

5-[3-Hydroxy-2-hydroxymethyl-propionamido)-N,N´-dimethyl-N,N´-bis-(2,3-dihydroxypropyl)-2,4,6-triiodoisophthalamide (iobitridol) is a nonionic X-ray contrast agent used in various radiologic procedures to aid the radiographic visualization of selected tissues or organs.

X-Ray imaging (planar and tomographic) techniques depend on tissue density differences that provide the image contrast produced by X-ray attenuation between the area of interest and surrounding tissues (1, 2). Contrast enhancement (opacification) with use of contrast agents increases the degree of contrast and improves the differentiation of pathologic processes from normal tissues. Because iodine, an element of high atomic density, causes high attenuation of X-rays within the diagnostic energy spectrum, water-soluble and reasonably safe iodinated contrast agents in intravenous injectable forms have been developed for clinical applications (3, 4).

Water-soluble, intravenous X-ray contrast agents are generally organic iodine compounds that contain one or more tri-iodinated benzene rings (5, 6). When injected intravenously, they are largely distributed in the extracellular fluid space and excreted unchanged by the kidneys (7). Contrast enhancement of a region of interest depends on the route of administration, delivery of the agent to the area by blood flow, and the final iodine concentration in the region. There are two basic types of these compounds: ionic and nonionic agents. The first monomeric ionic compound, in the form of 2,4,6-triiodobenzene acetrizoic acid, was synthesized by Wallingford (3). Most ionic contrast agents are derived from the basic structures of 3,5-diamino-2,4,6-triiodobenzoic acid, 5-amino-2,4,5-triiodoisophthalic acid, or 2,4,6-triiodobenzene-1,3,5-tricarbonic acid. In addition to monoacidic ionic dimers, nonionic compounds have also been developed to improve the tolerability of these agents in patients. The basic strategy of developing nonionic agents is to eliminate the electrical charges in the structure, which will lead to a reduction in osmolality of the compound. Because osmolality is related to the number of particles in solution, the challenge is to reduce the number of particles but maintain the iodine concentration (8). This was generally achieved by conversion of the carboxyl groups to hydroxyalkylamide groups (9).

As a low-osmolar nonionic monomer, iobitridol was developed in an effort to increase the safety and tolerance of X-ray contrast agents. The development of iobitridol was based on the belief that shielding of the hydrophobic areas of the 1,3,5-triiodobenzene ring from interaction with biological sites in vivo would decrease the chemotoxicity of this class of compounds (10-12). This compound is characterized by the introduction of a methyl group as second substituent in the tertiary amido group of the benzamide substituent chains to decrease the flexibility of the polar side-chains and to stabilize the hydrophilic sphere. However, Violon (13) compared iobitridol with four other nonionic monomers based on semi-empirical quantum mechanical calculations alone and concluded that the structured did not seem to stabilize the hydrophilic sphere to a greater extent than other studied molecules. Iobitridol is not commercially available in the United States but is available (http://www.guerbet.com/index.php?id=ourproducts&L=0) (250-350 mg iodine(I)/ml) in Europe for angiography, venography, and computed tomography (CT) examinations.

## Synthesis

PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Iobitridol%20OR%20Xenetix%29%20AND%20synthesis)]

The processes involved in the production of X-ray contrast agents are well-established organic reactions (5). Hoey et al. (14) described the basic approach of synthesizing derivatives of isophthalamic acid as contrast agents. Schaefer et al. (15) reported the synthesis of iobitridol from 5-[2-isopropyl-1,3-dioxanne-5-carboxamido]-2,4,6-triiodoisophtaloyle dichloride. The compound was suspended in isopropanol and triethylamine to react with N-methyl-aminopropane-2,3-diol for 12 h at room temperature. The obtained product (68.5% yield) was then dissolved in 5 N hydrochloric acid and stirred for 12 h at room temperature. After filtering and evaporation, the final product was obtained with a yield of 90%.

## In Vitro Studies: Testing in Cells and Tissues

PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28Iobitridol%20OR%20Xenetix%29%29%20AND%20%28%22in%20vitro%22%29)]

Using in vitro experimental models, Idee et al. (16) tested iobitridol at an iodine dosage of 350 mg/ml. Studies of cardiac and pulmonary effects were carried out on hearts of New Zealand rabbits and the isolated guinea pig lung model. A transient decrease in myocardial contractility and a transient increase in pulmonary perfusion/ventilation pressure were observed. Similar effects were observed with another nonionic contrast agent, iohexol. The toxicity of iobitridol, as tested in vitro with human blood and cultured fibroblasts (red blood cell (RBC) morphology, RBC osmotic fragility and hemolysis, and fibroblast cell death) was similar to that of iohexol. Iobitridol showed slight histamine-releasing activity at the150 mg I/ml concentration. Donandieu et al. (17) reported no mutagenic or clastogenic activity for iobitridol, based on tests in bacteria and in vitro human lymphocyte metaphase analysis.

Dencausse et al. (18), using ultracentrifugation, determined that the in vitro human albumin binding of iobitridol was 2.1%. In vitro metabolism studies of iobitridol were performed with (rat, monkey, dog, rabbit, and human) hepatic microsomes. Depending on the species, one, two, or three metabolites were detected, and each metabolite constituted no more than 1.9% of injected dose (ID). There was only one metabolite in monkeys, dogs, and rabbits, but there were two metabolites in humans and three metabolites in rats.

## Animal Studies

### Rodents

PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Iobitridol%20OR%20Xenetix%29%20AND%20rodentia)]

Using ^125^I-labeled iobitridol (specific activity = 166.5 MBq (4.5 mCi)/mg) and whole-body quantitative autoradiography, Bourrinet et al. (19) studied the biodistribution of iobitridol in rats. The administered dose was 3.7 MBq (0.1 mCi) in a dose of 300 mg I/kg. At 1 h after administration, the tissue/plasma radioactivity ratios were 29.56 (unblocked thyroid), 11.80 (kidneys), 1.90 (skin), 1.28 (lungs), 1.18 (liver), and 0.62 (heart). Radioactivity in the brain was not detectable. By 24 h after administration, radioactivity was detected only in the thyroid. The major excretion organ was the kidneys, with 86% ID was eliminated in 24-48 h. Only 5% ID was excreted via the fecal route. Dencausse et al. (18) performed pharmacokinetic studies of 300 mg I/kg iobitridol in rats (n = 6) and determined the following parameters: elimination half-time ((t_½β_); 25 ± 1 min), mean residence time (36 ± 2 min), apparent distribution volume (236 ± 11 ml/kg), and clearance (2 ± 0 ml/min).

Idee et al. (16) reported the renal effects of iobitridol at the dose of 1 ml/min (350 mg I/ml) for 3 min in rats. Forty-eight hours after injection, Iobitridol appeared to induce fewer histologic lesions (vacuolization of tubular cells) than iohexol. Iobitridol also showed similar nociceptive effects of intra-arterial injections in rats. Tervahartiala et al. (20) studied the structural changes in the rat renal proximal tubular cells induced by iobitridol, iopamidol, and iohexol. Rats were deprived of water 24 h before injection of contrast agents at a dosage of 3 g I/kg. By 2 h after injection, iopamidol had induced moderate changes, but both iohexol and iobitridol had induced prominent lysosomal alterations. These changes induced by iobitridol had almost disappeared after 48 h.

Donandieu et al. (17) studied the toxicologic profile of iobitridol. The acute i.v. toxicity lethal dose (LD_50_) of iobitridol (350 mg I/ml) in mice was 15.9 g I/kg. In comparison, the LD_50_ for iohexol was also 15.9 I/kg. No acute oral toxicity was observed in mice up to 17.5 g I/kg. No deaths were observed after intracisternal injection. Subacute toxicity did not lead to any deaths in the rats at dosages up to 3.5 g I/kg/day for 28 days. No indication of embryo-fetal toxicity was observed in rats. No clastogenic activity was demonstrated through the micronucleus test in mice.

### Other Non-Primate Mammals

PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Iobitridol%20OR%20Xenetix%29%20AND%20%28dog%20OR%20pig%20OR%20rabbit%20OR%20sheep%29)]

Dencausse et al. (18) performed pharmacokinetic studies of 300 mg I/kg iobitridol in rabbits (n = 6) and determined the following parameters: elimination t_½β_ (72 ± 6 min), mean residence time (90 ± 5 min), apparent distribution volume (267 ± 18 ml/kg), and clearance (7 ± 0 ml/min). The excretion was 92 ± 5% via urine and 0.73 ± 0.1% via feces in 24 h. In dogs (n = 6), these parameters were as follows: elimination t_½β_ = 53 ± 3 min, mean residence time = 66 ± 4 min, apparent distribution volume = 252 ± 11 ml/kg, and clearance = 45 ± 3 ml/min. The excretion was 91 ± 2% via urine and 0.16 ± 0.03% via feces in 5 h.

Idee et al. (16) studied the in vivo bronchopulmonary effects, cardiopulmonary/renal effects, and neurologic effects of iobitridol in different animal models. No bronchospasms were observed in the guinea pig model. Cardiopulmonary and renal effects of iobitridol were similar to those of iohexol in dogs. No blood-brain barrier damage caused by iobitridol was observed in rabbits.

Donandieu et al. (17) reported no deaths and no systemic clinical toxicity signs after i.v. and perivenous injections of iobitridol in rabbits. Iobitridol appears to provoke only minimal reversible local reactions. No indication of teratogenicity was found in rabbits with iobitridol doses up to 3.5 g I/kg. No deaths were reported in dogs treated daily with iobitridol at doses up to 2.8 g I/kg.

### Non-Human Primates

PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Iobitridol%20OR%20Xenetix%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Iobitridol%20OR%20Xenetix%29%20AND%20humans)]

Fournier et al. (21) evaluated the clinical safety and efficacy of iobitridol (350 mg I/ml) on 60 patients who underwent intravenous urography. The dose was 1 ml/kg up to a maximum total dose of 200 ml. The reported events were all very mild. There were 11 (18.3% of 60 patients) events of early, including transient warm sensation, and 2 events (3.3%) of nausea and vomiting. Image quality of iobitridol was judged to be good or excellent in 72-74% of the cases.

In a randomized double-blind phase III study, Hoogewoud and Woessmer (22) reported on the clinical safety of iobitridol (300 mg I/ml) compared with another monomeric nonionic contrast agent, iopromid, in 60 patients who had abdominal CT. They found that both iobitridol and iopromide provided similar image quality and side effects. Bach et al. (23) studied the effects of iobitridol on downstream capillary perfusion in a prospective, randomized, double-blind phase IV clinical trial. The study examined the cutaneous microcirculation in patients who underwent diagnostic cardiac catheter examination. The capillary erythrocyte velocity (V_RBC_) was measured before and up to 3 min after the injection of the contrast agent. The mean difference in V_RBC_ between the baseline value and the maximum decrease after injection (V_diff-max_) of iobitridol (350 mg I/ml) was –0.07 mm/s in 10 patients. In comparison, the V_diff-max_ values for iopromide (370 mg I/ml) and iodixanol (320 mg I/ml); a dimeric, nonionic contrast agent) were –0.23 and –0.22, respectively. The authors suggested that the microcirculatory disturbance induced by iobitridol was less severe than with other nonionic contrast agents.

Vogl et al. (24) reviewed the rate of adverse events associated with iobitridol in the general patient population and at-risk patients. The review included 210 radiologists who conducted various examinations in 52,057 patients. The adverse event rates were 0.96% and 1.39% for all patients and at-risk patients, respectively. The most frequent adverse events were sensation of heat (0.31%), nausea (0.24%), and urticaria (0.12%). The frequencies of all other events were less than 0.01%. The serious event rate was 0.044% in all patients and 0.057% in at-risk patients. These serious events included dyspnea (0.033%), hypotension (0.008%), and anaphylactic shock (0.006%). Petersein et al. (25) reported the results of a postmarketing surveillance study with iobitridol at various doses (1.5% of patients receiving 250 mg I/kg, 92.7% receiving 300 mg I/kg, and 5.8% receiving 350 mg I/kg) in 61,754 patients from 1996 to 2000. The adverse event rate was 2.3% of all of the examinations. The most frequent events were feeling of warmth (2.3%), nausea (1.3%), and urticaria (0.1%). Subjective assessment of image quality indicated that 99.0% of 60,021 examinations were diagnostic. Image quality assessment indicated that images were excellent or good in 90.5% and 90.6% of normal weight and overweight patients, respectively.

Various other studies [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Iobitridol%20OR%20Xenetix%29%20AND%20%28Clinical%20Trial%29)] have indicated that iobitridol is at least as safe and effective as other commercially available nonionic contrast agents.

## Supplemental Information

[Disclaimers]

Iobitridol products.

## References

1 Swanson, D.P. and M.B. Alpern, Contrast media for computed tomography: Intravascular, intracavitary, xenon, reticuloendothelial, in Pharmaceuticals in medical imaging, D.P. Swanson, H. M. Chilton and J. H. Thrall, Editor. 1990, Macmillan Publishing Company: New York. p. 99-124.
2 Hoey, G.B. and K.R. Smith, Chemistry of X-ray contras media, in Radiocontrast agents, M. Sovak, Editor. 1984, Springer-Verlag: New York. p. 23-125.
3 Wallingford V.H. (1953). The development of organic iodine compounds as x-ray contrast media. J Am Pharm Assoc Am Pharm Assoc Baltim.
4 Sovak, M., R. Ranganathan, J.H. Lang, and E.C. Lasser, Concepts in design of improved intravascular contrast agents. European Society of cardiovascular Radiology, Uppsala, 1977(May): p. 25-27.
5 Gries, H., Chemistry of X-ray contrast agents, in Textbook of contrast media, P. Dawson, D.O. Cosgrove, and R.G. Grainger, Editors. 1999, Isis Medical Media Ltd.: Oxford. p. 15-22.
6 Almen T. (1969). Contrast agent design. Some aspects on the synthesis of water soluble contrast agents of low osmolality. J Theor Biol.
7 Dawson, P., Pharmacokinetics of water-soluble iodinated X-ray contrast agents, in Textbook of contrast media, P. Dawson, D.O. Cosgrove, and R.G. Grainger, Editors. 1999, Isis Medical Media Oxford. p. 61-74.
8 Ralston W.H., Robbins M.S., Coveney J., Blair M. (1989). Acute and subacute toxicity studies of ioversol in experimental animals. Invest Radiol.
9 Almen T. Development of nonionic contrast media Invest Radiol 1985 20Suppl1 S2 9 2579043
10 Meyer D., Petta M., Fouchet M.H., Vadel M., Schaefer M., Dugast-Zrihen M., Guillemot M. (1996). Stabilization of the hydrophilic sphere of iobitridol, a new nonionic iodinated contrast agent. Acta Radiol Suppl.
11 Carrupt P.A., Testa B. (2003). Stabilization of the hydrophilic sphere of iobitridol. Br J Radiol.
12 Meyer D., Fouchet M.H., Petta M., Carrupt P.A., Gaillard P., Testa B. (1995). Stabilization of the hydrophilic sphere of iobitridol, an iodinated contrast agent, as revealed by experimental and computational investigations. Pharm Res.
13 Violon D. (2001). Stabilization of the hydrophilic sphere of non-ionic monomers: are all protected in a similar way?. Br J Radiol.
14 Hoey G.B. Rands R.D. DeLaMater G. Chapman D.W. Wiegert P.E. Synthesis of derivatives of isophthalamic acid as X-ray contrast agents. 1963
15 Schaefer M. D.-Z. D.-Z. M. Guillemot M. Doucet D. Meyer D. Iodinated non-ionic triiodobenzene compounds and contrast media containing them, U.S. Patent Number 5,043,1521991, United States Patient Office: U.S. p. 1-13.
16 Idee J.M., Bault C., Beaufils H., Berthommier C., Cambar J., Corot C., Doucet D., Hartl C., Jaudon M.C., Jacquiaud C., Lakhdar B., Potier M., santus R., Torcherie S., Vaudon E., Bonnemain B. (1996). Pharmacologic profile of iobitridol, a nonionic iodinated contrast medium. Acta Radiol Suppl.
17 Donandieu A.M., Idee J.M., Doucet D., Legros A., Penati S., Nain-Dit-Ducret M., Marmion F., Bonnemain B. (1996). Toxicologic profile of iobitridol, a new nonionic low-osmolality contrast medium. Acta Radiol Suppl.
18 Dencausse A., Violas X., Feldman H., Havard P., Chambon C. (1996). Pharmacokinetic profile of iobitridol. Acta Radiol Suppl.
19 Bourrinet P., Dencausse A., Cochet P., Bromet-Petit M., Chambon C. (1994). Whole body quantitative autoradiographic study of the biodistribution of iobitridol in rats. Invest Radiol.
20 Tervahartiala P., Kivisaari L., Kivisaari R., Vehmas T., Virtanen I. (1997). Structural changes in the renal proximal tubular cells induced by iodinated contrast media. Nephron.
21 Fournier P.J., Steinbrich W., Freitag P., Voegeli E. (1996). Evaluation of the clinical safety and efficacy of iobitridol (Xenetix) in intravenous urography. Eur J Radiol.
22 Hoogewoud H.M., Woessmer B. (1996). Iobitridol 300 compared to iopromide 300--a double-blind randomized phase-III study of clinical tolerance in total body CT. Acta Radiol Suppl.
23 Bach R., Gerk U., Mrowietz C., Jung F. (2000). Influence of a new monomeric nonionic radiographic contrast medium (iobitridol-350 versus NaCl) on cutaneous microcirculation: single-center, prospective, randomized, double-blind phase IV study in parallel group design. Microvasc Res.
24 Vogl T.J., Honold E., Wolf M., Mohajeri H., Hammerstingl R. (2006). Safety of iobitridol in the general population and at-risk patients. Eur Radiol.
25 Petersein J., Peters C.R., Wolf M., Hamm B. (2003). Results of the safety and efficacy of iobitridol in more than 61,000 patients. Eur Radiol.